# 5-Amino-7-(3-(4-[^11^C]methoxy)phenylpropyl)-2-(2-furyl)pyrazolo[4,3-e]-1,2,4-triazolo[1,5-c]pyrimidine

Chemical name: | 5-Amino-7-(3-(4-[^11^C]methoxy)phenylpropyl)-2-(2-furyl)pyrazolo[4,3-e]-1,2,4-triazolo[1,5-c]pyrimidine
Abbreviated name: | [^11^C]SCH442416
Synonym:
Agent Category: | Compound
Target: | Adenosine A_2A_ receptor
Target Category: | Receptor binding
Method of detection: | PET
Source of signal: | ^11^C
Activation: | No
Studies: | - In vitro; - Rodents; - Non-human primates | Click on the above structure for additional information in PubChem (http://pubchem.ncbi.nlm.nih.gov).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=SCH442416)]

Adenosine is an endogenous nucleoside that modulates a number of physiologic functions in the central nervous system (CNS) and in peripheral organs such as the heart, kidney, and muscle (1, 2). The effect is mediated by two major subtypes of receptors (A_1_ and A_2A_ receptors) and two minor subtypes (A_2B_ and A_3_). In the CNS, A_1_ receptors are present both pre- and post-synaptically in the hippocampus, cerebral cortex, thalamus, striatum, and cerebellum. A_2A_ receptors are highly concentrated and co-localized with dopamine D_1_ and D_2_ receptors in the striatum, nucleus accumbens, and olfactory tubercle. A_2A_ receptors are also present in low levels in the hippocampus and cortex. A_2B_ receptors are widely distributed, but the density is higher in the gastrointestinal tract. A_3_ receptors are also widely distributed but with higher density in the testis. A_1_ and A_3_ receptors mediate inhibition of adenylyl cyclase, whereas A_2A_ and A_2B_ receptors mediate stimulation. Changes in the adenosine receptor functions are implicated in epilepsy, ischemic cerebral stroke, movement disorders, sleep disorders, and psychiatric disorders (3-5).

A_2A_ receptors have been studied in vivo by positron emission tomography (PET) using [7-methyl-^11^C]-(E)-8-(3,4,5-trimethoxystyryl)-1,3,7-trimethylxanthine ([^11^C]TMSX), a methylxanthine analog of KF17387 with selective A_2A_ antagonistic activity (6). TMSX showed better selectivity for A_2A_ over A_1_ receptors than KF17387 and had little affinity in various neuroreceptor-binding assays (7). However, TMSX as a xanthine analog is subject to photoisomerization. 5-Amino-7-(3-(4-methoxy)phenylpropyl)-2-(2-furyl)pyrazolo[4,3-e]-1,2,4-triazolo[1,5-c]pyrimidine, a non-xanthine derivative of pyrazolo[4,3-e]-1,2,4-triazolo[1,5-c]pyrimidine, is found to be a selective and potent antagonist for the A_2A_ receptors (8). 5-Amino-7-(3-(4-[^11^C]methoxy)phenylpropyl)-2-(2-furyl)pyrazolo[4,3-e]-1,2,4-triazolo[1,5-c]pyrimidine ([^11^C]SCH442416) is being developed as a PET agent for the non-invasive study of A_2A_ receptors in the human brain.

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=SCH442416+and+synthesis)]

In the report by Todde et al. (8), [^11^C]SCH442416 was synthesized by the direct methylation of the phenol precursor with [^11^C]methyl iodide in dimethylformamide in the presence of sodium hydroxide at 90°C for 4 min. Purification by high-performance liquid chromatography and solid phase extraction provided a decay-corrected radiochemical yield of 28.7 ± 7.2%, radiochemical purity >96%, and specific activity of 55.13 ± 36.26 GBq/μmol (1.49 ± 0.98 Ci/μmol) at the end of synthesis. The total synthesis time was 40 min.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=SCH442416+and+in+vitro)]

In the receptor-binding studies by Todde et al. (8), the K_i_ values of SCH442416 were 0.048 nM for the A_2A_ receptors, >10,000 for A_2B_ and A_3_, and 1,111 nM for the A_1_ receptors. Hence, SCH442416 showed good selectivity for A_2A_ receptors. SCH442416 is more potent in inhibiting A_2A_ receptor binding than TMSX (K_i_ = 5.9 nM). Saturation binding experiments of [^11^C]TMSX in the rat striatum and cortex gave estimated B_max_ values of 170 and 33 fmol/mm^3^ tissue, respectively (7).

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=SCH442416+and+rodentia)]

Biodistribution studies by Todde et al. (8) showed high initial accumulation of radioactivity in the liver (0.94 ± 0.17% injected dose (ID)/g), followed by the adrenal gland (0.85 ± 0.33% ID/g), kidney (0.69 ± 0.09% ID/g), and lung (0.38 ± 0.11% ID/g) at 5 min after injection of [^11^C] SCH442416 in normal rats. The levels of radioactivity were low in the brain (<0.2% ID/g) and blood (0.13% ID/g). Radioactivity levels decreased gradually in all studied organs. Regional brain biodistribution showed that the striatum had a maximum uptake (0.46 ± 0.10% ID/g) at 5-15 min after injection, whereas the accumulation levels in the cerebellum (0.19 ± 0.04% ID/g) and cortex (0.19 ± 0.04% ID/g) were lower. The striatum/cerebellum ratio was 4.6 ± 0.27 at 15 min and 4.0 ± 0.85 at 30 min. ~70% and >94% of radioactivity in the plasma and brain, respectively, was intact [^11^C]SCh442416 at 15 min post injection. Two hydrophilic metabolites were found in the plasma with ~60% of the intact tracer at 60 min. Moresco et al. (9) showed that pre-administration of the A_2A_ selective (SCH 442416, SCH58261, and KW6002) or non-selective antagonists (caffeine), but not the A_1_ (DPCPX) or D_1_ (SCH23390) or D_2_ antagonists (FESP), significantly decreased the accumulation in the striatum at 15 min after injection.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=SCH442416+and+(dog+or+pig+or+sheep+or+rabbit))]

No publications are currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=SCH442416+and+(primate+not+human))]

Using PET, Moresco et al. (9) obtained serial brain scans in 1 monkey after injection of 30 MBq (0.81 mCi) of [^11^C]SCH442416. The accumulation of radioactivity in the striatum (0.035% ID/ml) peaked at 2-4 min after injection and then decreased for the final 60 min of study. The striatum/cerebellum ratios reached a maximum value of 2.2 at 15 min and 1.5 at 60 min. The striatum was estimated to have a binding potential of 0.74 ± 0.02 with a simplified reference tissue model (the cerebellum as input function). Mihara et al. (10) measured the adenosine A_2A_ receptor occupancy in rhesus monkeys (n = 3) after the administration of various doses of A_1_/A_2A_ receptor antagonist ASP5854 using ^11^C-SCH442416 PET imaging. The occupancy for adenosine A_2A_ receptors in the caudate was 9.0% (0.001 mg/kg), 50.7% (0.01 mg/kg), and 87.4% (0.1 mg/kg).

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=SCH442416+and+human)]

No publications are currently available.

## References

1 Fredholm B.B., Abbracchio M.P., Burnstock G., Daly J.W., Harden T.K., Jacobson K.A., Leff P., Williams M. (1994). Nomenclature and classification of purinoceptors. Pharmacol Rev.
2 Palmer T.M., Stiles G.L. (1995). Adenosine receptors. Neuropharmacology.
3 Dunwiddie T.V., Masino S.A. (2001). The role and regulation of adenosine in the central nervous system. Annu Rev Neurosci.
4 El Yacoubi M. Costentin J. Vaugeois J.M. Adenosine A2A receptors and depression Neurology 2003 61Suppl 611 S82 7 14663017
5 von Lubitz D.K. (2001). Adenosine in the treatment of stroke: yes, maybe, or absolutely not?. Expert Opin Investig Drugs.
6 Noguchi J., Ishiwata K., Wakabayashi S., Nariai T., Shumiya S., Ishii S., Toyama H., Endo K., Suzuki F., Senda M. (1998). Evaluation of carbon-11-labeled KF17837: a potential CNS adenosine A2a receptor ligand. J Nucl Med.
7 Ishiwata K., Ogi N., Shimada J., Nonaka H., Tanaka A., Suzuki F., Senda M. (2000). Further characterization of a CNS adenosine A2a receptor ligand [11C]KF18446 with in vitro autoradiography and in vivo tissue uptake. Ann Nucl Med.
8 Todde S., Moresco R.M., Simonelli P., Baraldi P.G., Cacciari B., Spalluto G., Varani K., Monopoli A., Matarrese M., Carpinelli A., Magni F., Kienle M.G., Fazio F. (2000). Design, radiosynthesis, and biodistribution of a new potent and selective ligand for in vivo imaging of the adenosine A(2A) receptor system using positron emission tomography. J Med Chem.
9 Moresco R.M., Todde S., Belloli S., Simonelli P., Panzacchi A., Rigamonti M., Galli-Kienle M., Fazio F. (2005). In vivo imaging of adenosine A2A receptors in rat and primate brain using [11C]SCH442416. Eur J Nucl Med Mol Imaging.
10 Mihara T., Noda A., Arai H., Mihara K., Iwashita A., Murakami Y., Matsuya T., Miyoshi S., Nishimura S., Matsuoka N. (2008). Brain Adenosine A2A Receptor Occupancy by a Novel A1/A2A Receptor Antagonist, ASP5854, in Rhesus Monkeys: Relationship to Anticataleptic Effect. J Nucl Med.